# (R)-2-Amino-3-[^18^F]fluoro-2-methylpropanoic acid

Chemical name: | (R)-2-Amino-3-[^18^F]fluoro-2-methylpropanoic acid
Abbreviated name: | (R)-[^18^F]FAMP
Synonym:
Agent category: | Compound
Target: | L-type and A-type amino acid transporter
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FAMP)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine, and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. There are also ^123^I-labeled amino acids used in imaging in oncology (4-6).The natural amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and retained in tumor cells because of their higher metabolic pathways, including incorporation into proteins, than most normal cells (4). L-[^11^C]Methionine and [^18^F]fluorotyrosine have been widely used in the detection of tumors. On the other hand, the non-natural amino acids are not metabolized. Their uptakes are through both the L-type transporter and the energy-dependent A-type transporter (7). Therefore, they can accumulate intracellularly in high concentrations. [^11^C]Aminoisobutyric acid was shown to have a high tumor/brain ratio (8, 9). (R)-2-Amino-3-[^18^F]fluoro-2-methylpropanoic acid ((R)-[^18^F]FAMP) is a fluorinated analog of [^11^C]α-aminoisobutyric acid (AIB) that is being evaluated as a useful tracer in PET tumor imaging (10).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20transporter+AND+micad%5Bbook%5D)
- Gene information in NCBI (Amino acid transporter (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=8140))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D)
- Clinical trials (Amino acid transporter (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporter))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+synthesis)]

Nucleophilic fluorination of (R)3-(tert-butoxycarbonyl)-4-methyl-1,2,3-oxathiazolidine-4-carboxylic acid tert-butyl ester 2,2-dioxide with K[^18^F]F/Kryptofix2.2.2 and subsequent hydrolysis and purification provided a radiosynthesis yield (decay-corrected) of 52% for (R)-[^18^F]FAMP at the end of bombardment. A radiochemical purity of 99% was obtained. The total synthesis time was 85 min. The specific activity was ~1.85 GBq/µmol (50 mCi/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+in+vitro)]

(R)-[^18^F]FAMP exhibited a rapidly increasing uptake into L9 rat gliosarcoma tumor cells with 13.06 ± 0.23% (n = 3) injected dose (ID)/5 × 10^5^ cells at 30 min of incubation (10). The uptake was blocked by the presence of L-type transporter inhibitor BCH (2-amino-bicyclo[2.2.1]heptane-2-carboxylic acid), A-type transporter inhibitor MeAIB (N-methyl-AIB), and system ASC inhibitor ACS (alanine-cysteine-serine) with 67%, 58%, and 87% inhibition, respectively. (S)-[^18^F]FAMP (4.77 ± 0.73% ID/5 × 10^5^ cells) exhibited a lower uptake than (R)-[^18^F]FAMP. The uptake was blocked by the presence of BCH, MeAIB, and ACS with 75%, 31%, and 72% inhibition, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+rodentia)]

Yu et al. (10) performed ex vivo biodistribution studies of (R)-[^18^F]FAMP in rats implanted intracerebrally with a 9L gliosarcoma. The uptake in the brain (0.06% ID/g) was low at 30 min after injection and increased slightly to 0.09% ID/g at 120 min. The uptake in the tumor was 2.42–2.82% ID/g at 30–120 min after injection. Most of the other tissues showed lower radioactivity levels at 120 min than at 30 min. The organs with the highest accumulation at 30 min were the pancreas (2.96% ID/g) and kidney (3.47% ID/g). The tumor/brain ratios were 38.2, 28.6, and 27.5 at 30, 60, and 120 min, respectively. The radioactivity in the bone was low (0.26% ID/g at 120 min). (S)-[^18^F]FAMP exhibited lower tumor accumulation (1.38–2.13% ID/g) but higher pancreas and kidney accumulation than (R)-[^18^F]FAMP. The tumor/brain ratios were 21.1, 30.9, and 27.7 at 30, 60, and 120 min, respectively. No blocking experiments were performed. The specificity of uptake, especially given the disruption of the blood brain barrier, was not studied.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FAMP%5BAll%20Fields%5D%20AND%20human)]

No publication is currently available.

## References

1 Coleman R.E., Hoffman J.M., Hanson M.W., Sostman H.D., Schold S.C. (1991). Clinical application of PET for the evaluation of brain tumors. J Nucl Med.
2 Kaschten B., Stevenaert A., Sadzot B., Deprez M., Degueldre C., Del Fiore G., Luxen A., Reznik M. (1998). Preoperative evaluation of 54 gliomas by PET with fluorine-18-fluorodeoxyglucose and/or carbon-11-methionine. J Nucl Med.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
5 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
6 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
7 Palacin M., Estevez R., Bertran J., Zorzano A. (1998). Molecular biology of mammalian plasma membrane amino acid transporters. Physiol Rev.
8 Conti P.S., Sordillo P.P., Schmall B., Benua R.S., Bading J.R., Bigler R.E., Laughlin J.S. (1986). Tumor imaging with carbon-11 labeled alpha-aminoisobutyric acid (AIB) in a patient with advanced malignant melanoma. Eur J Nucl Med.
9 Fross R.D., Warnke P.C., Groothuis D.R. (1991). Blood flow and blood-to-tissue transport in 9L gliosarcomas: the role of the brain tumor model in drug delivery research. J Neurooncol.
10 Yu W., McConathy J., Williams L., Camp V.M., Malveaux E.J., Zhang Z., Olson J.J., Goodman M.M. (2010). Synthesis, radiolabeling, and biological evaluation of (R)- and (S)-2-amino-3-[(18)F]fluoro-2-methylpropanoic acid (FAMP) and (R)- and (S)-3-[(18)F]fluoro-2-methyl-2-N-(methylamino)propanoic acid (NMeFAMP) as potential PET radioligands for imaging brain tumors. J Med Chem.